# 4-Acetoxy-7-chloro-3-(3-(-4-[^11^C]methoxybenzyl)phenyl)-2(1H)-quinolone

Chemical name: | 4-Acetoxy-7-chloro-3-(3-(-4-[^11^C]methoxybenzyl)phenyl)-2(1H)-quinolone
Abbreviated name: | [^11^C]AcL703,717, [^11^C]AcL703
Synonym:
Agent category: | Compound
Target: | N-Methyl D-aspartate (NMDA) receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703)]

N-Methyl D-aspartate (NMDA) receptor is an ionotropic receptor for glutamate playing an important role in synaptic plasticity, which is a cellular mechanism for learning and memory (1). The NMDA receptor forms a heterotetramer between two NR1 and two NR2 subunits with multiple regulatory binding sites for glutamate, glycine, Mg^2+^, polyamine, and drugs such as phencyclidine (PCP) (2). Overactivation of NMDA receptor has been suggested to be involved in a variety of neurological diseases such as ischemia, schizophrenia, Parkinson’s disease, Huntington’s disease, and epilepsy.

4-Hydroxy-7-chloro-3-(3-(-4-methoxybenzyl)phenyl)-2(1H)-quinolone (L703,717), a 4-hydroxyquinolone, is a potent antagonist for the glycine-binding site of the NMDA receptor, but it is poorly taken up by the brain because of its tight binding to serum albumin (3). Haradahira et al. (4) introduced an ester to the 4-hydroxyquinolone moiety to improve its penetration through the blood–brain barrier. 4-Acetoxy-7-chloro-3-(3-(-4-methoxybenzyl)phenyl)-2(1H)-quinolone (AcL703,717) taken up by the brain can be expected to be hydrolyzed to L703,717 by esterase in the brain. [^11^C]AcL703,717 is being evaluated as a positron emission tomography (PET) radioligand to study NMDA receptor in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20synthesis)]

[^11^C]AcL703,717 was prepared in two-step reactions (4). The desmethyl precursor of L703,717 was reacted with [^11^C]methyl iodide in the presence of NaH in dimethylformamide for 3 min at 30°C. Subsequently, the acetylation was performed by addition of acetic anhydride/2,6-lutidine to the mixture, which was heated for 3 min at 80°C. [^11^C]AcL703,717 was obtained with a radiochemical purity of >99% and a specific radioactivity of 51–73 GBq/µmol (1.38–1.97 Ci/µmol) at the end of synthesis. The total synthesis time was 33 min from the end of bombardment. [^11^C]AcL703,717 exhibited a Log P value of 3.9, whereas [^11^C]L703,717 had a Log P value of 3.0.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20in%20vitro)]

Haradahira et al. (4) reported that 80% of [^11^C]AcL703,717 was converted to [^11^C]L703,717 by incubation with the rat brain homogenates for 20 min. No other metabolites were detected. [^11^C]AcL703,717 was stable in saline buffer under the experimental conditions used. However, [^11^C]AcL703,717 was readily converted to [^11^C]L703,717 by incubation with the rat and mouse plasma (4) as well as in human blood (5) with a half-life of <1 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

[^11^C]AcL703,717 (8 MBq (216 μCi)) was injected intravenously into normal mice to study its accumulation in the brain at 1 min after injection (4). [^11^C]AcL703,717 showed an initial penetration into the brain with 0.71 ± 0.10% injected dose (ID)/g in the cerebellum and 0.58 ± 0.05% ID/g in cerebrum. The initial radioactivity levels in the brain were one-fold higher than those of [^11^C]L703,717. There was <10% of intact [^11^C]AcL703,717 in the brain at 5 min after injection with [^11^C]L703,717 as the only metabolite. Ex vivo brain autoradiography at 20 min after injection of [^11^C]AcL703,717 showed that the main radioactivity in the cerebellum was similar to that of [^11^C]L703,717. This cerebellar radioactivity was completely blocked with co-injection of L703,717 (1 mg/kg). Ex vivo brain autoradiography studies of the rat brain showed that pretreatment with cyclosporine, a P-gp inhibitor, increased the cerebellar radioactivity of [^11^C]AcL703,717 one-fold. The authors mentioned that it is not clear whether most of the [^11^C]L703,717 is formed in the brain or formed in the blood and then cross the BBB as the [^11^C]L703,717 to account for the increase brain accumulation of [^11^C]AcL703,717 over [^11^C]L703. No blocking experiment with L703,717 was presented.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20%22animals%22%5BMeSH%5D%20NOT%20%22rodentia%22%5BMeSH%20Terms%5D%20NOT%20%22primates%22%5BMeSH%5D)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20%22primates%22%5BMeSH%5D%20NOT%20%22humans%22%5BMeSH%5D)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ACL703%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

Matsumoto et al. (5) performed dynamic PET scans in six healthy male volunteers (23.3 ± 2.9 years old) for 90 min after injection of 624–851 MBq (17–23 mCi) [^11^C]AcL703,717. The maximum whole-brain accumulation was 1.3% at 1.5 min after injection. The brain region with the highest radioactivity accumulation at 40–90 min after injection was the cerebellar cortex, followed by the frontal-temporal-parietal cortex, thalamus, striatum, and white matter. The binding potential (BP) values (white matter as reference region) for the cerebellar cortex and frontal-temporal-parietal cortex were calculated to be 2.2 ± 0.71 and 1.05 ± 0.45, respectively. The BP values for thalamus and striatum were almost zero.

## References

1 Bear M.F. (1996). A synaptic basis for memory storage in the cerebral cortex. Proc Natl Acad Sci U S A.
2 McBain C.J., Mayer M.L. (1994). N-methyl-D-aspartic acid receptor structure and function. Physiol Rev.
3 Haradahira T., Suzuki K. (1999). An improved synthesis of [11C]L-703,717 as a radioligand for the glycine site of the NMDA receptor. Nucl Med Biol.
4 Haradahira T., Zhang M.R., Maeda J., Okauchi T., Kida T., Kawabe K., Sasaki S., Suhara T., Suzuki K. (2001). A prodrug of NMDA/glycine site antagonist, L-703,717, with improved BBB permeability: 4-acetoxy derivative and its positron-emitter labeled analog. Chem Pharm Bull (Tokyo).
5 Matsumoto R., Haradahira T., Ito H., Fujimura Y., Seki C., Ikoma Y., Maeda J., Arakawa R., Takano A., Takahashi H., Higuchi M., Suzuki K., Fukui K., Suhara T. (2007). Measurement of glycine binding site of N-methyl-D-asparate receptors in living human brain using 4-acetoxy derivative of L-703,717, 4-acetoxy-7-chloro-3-[3-(4-[11c] methoxybenzyl) phenyl]-2(1H)-quinolone (AcL703) with positron emission tomography. Synapse.